# Radioiodinated (1E,4E)-1-(4-aminophenyl)-5-(4-iodophenyl)penta-1,4-dien-3-one and (1E,4E)-1-(4-iodophenyl)-5-(4-(methylamino)phenyl)penta-1,4-dien-3-one

Chemical name: | Radioiodinated (1E,4E)-1-(4-aminophenyl)-5-(4-iodophenyl)penta-1,4-dien-3-one and (1E, 4E)-1-(4-iodophenyl)-5-(4-(methylamino)phenyl)penta-1,4-dien-3-one | [image]
Abbreviated name: | [^125^I]70, [^125^I]71 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^125^I]70 and [^125^I]71 by Cui et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

Radioiodinated (1E,4E)-1-(4-aminophenyl)-5-(4-iodophenyl)penta-1,4-dien-3-one (compound 70) and (1E, 4E)-1-(4-iodophenyl)-5-(4-(methylamino)phenyl)penta-1,4-dien-3-one (compound 71), abbreviated as [^125^I]70 and [^125^I]71, respectively, are two dibenzylideneacetone derivatives synthesized by Cui et al. for single-photon emission computed tomography (SPECT) of Alzheimer’s disease (AD) by targeting β-amyloid (Aβ) plaques (1).

AD is characterized in pathology by the presence of extracellular Aβ plaques, intraneuronal neurofibrillary tangles, and neuronal loss in the cerebral cortex (2, 3). Of them, Aβ deposit is the earliest neuropathological marker and is relatively specific to AD and closely related disorders. Aβ plaques are composed of abnormal paired helical filaments 5–10 nm in size. These filaments are largely made of insoluble Aβ peptides that are 40 or 42 amino acids in length (4). Aβ peptides have been shown to be toxic to neurons, and the level of Aβ peptides is closely correlated with the cognitive decline in AD. These features of Aβ prompted investigators to develop Aβ-targeted agents for AD imaging.

Curcumin is the principal component of the Indian spice turmeric, and in structure it is composed of two aromatic rings connected by two α,β-unsaturated carbonyl groups (1). In 2001, investigators at the University of California, Los Angeles, reported that curcumin is effective against neurodegeneration, oxidative damage, and diffuse plaque deposition after Aβ infusion in animals (5, 6). The anti-AD effect of curcumin has been further demonstrated to be partially due to its specific binding with Aβ, whereby it could break apart Aβ aggregates. In 2006, Ryu et al. tested eight curcumin derivatives as Aβ-specific imaging probes (7). In general, these derivatives are poor in brain–blood barrier (BBB) penetration and are unstable in vivo (1, 7). The curcumin derivatives are quickly converted to unidentified polar products, which cannot cross the BBB. The methylene moiety between the two aromatic rings is responsible for the poor stability, whereas the two aromatic rings are responsible for the binding with Aβ plaques. To improve the stability and BBB-penetrating ability of curcumin, various modifications on the curcumin structure have recently been made, including deleting the active methylene moiety in the middle of its structure (1).

Cui et al. synthesized a series of dibenzylideneacetones by deleting the methylene moiety and one carbonyl moiety and further linking various substituents on one (forming an asymmetrical structure) or on both aromatic rings (forming a symmetrical structure) (1). Analysis of the structure–affinity relationship among these derivatives has shown that dibenzylideneacetone without any substituents have a weak affinity with Aβ (inhibition constant (K_i_) = 242.5 ± 42.8 nM). Introduction of Cl or methoxy groups at the para position on both phenyl rings to form symmetrical ligands can significantly increase the binding affinity (~90 folds), and the size of substituents has no effect on the affinity for Aβ aggregates. Methylation of a primary amino group to form a secondary or tertiary amino group can also significantly increase the affinity (e.g., the agents [^125^I]70 and [^125^I]71 described in this chapter), but methylation of the amino group at the ortho position reduces the binding affinity dramatically. Increasing the substituent size at the aromatic amino group also leads to decreased binding affinity. However, when a phenyl ring in the dibenzylideneacetone structure is changed to a heterocyclic ring, such as a thiophene, furan, pyridine, or pyrrole ring, the generated compounds maintain the high binding affinity. These results demonstrate that the para position is highly tolerant of steric bulk substitutions, which opens up the possibility of developing new, easily labeled radioligands for imaging Aβ plaques in vivo (1).

This chapter summarizes the data obtained with [^125^I]70 and [^125^I]71, two asymmetrical dibenzylideneacetones with methylation of a primary amino group at the para position (1). Another chapter summarizes the data obtained with [^18^F]83 and [^18^F]85, two fluoro-pegylated dibenzylideneacetones.

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

Synthesis of compounds 70 and 71 was described in detail by Cui et al. (1). The radioiodinated ligands [^125^I]70 and [^125^I71 were prepared from the corresponding tributyltin precursors through iododestannylation reaction with hydrogen peroxide as an oxidant. The two agents were purified, and their radiochemical identities were verified with high-performance liquid chromatography. For the final products [^125^I]70 and [^125^I]71, their radiochemical yields were 15.3% and 24.1%, respectively, and their radiochemical purities were >98%. The specific activity of the no carrier-added preparation was comparable to that of Na^125^I (2,200 Ci/mmol (81.4 TBq/mmol)). The partition coefficients of [^125^I]70 and [^125^I71 were 3.26 and 3.55, respectively, indicating that both agents were lipophilic.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

The binding affinity of unlabeled compounds 70 and 71 for Aβ_1_−_42_ was examined with [^125^I]IMPY (6-iodo-2-(4'-dimethylamino)phenyl-imidazo[1,2]pyridine) as the competing radioligand (1, 8). The K_i_ values of compounds 70 and 71 were 7.0 ± 2.2 nM and 2.8 ± 0.5 nM, respectively, which was superior to the binding affinity of IMPY (K_i_ = 10.5 nM) (8).

The binding of [^125^I]71 to Aβ plaques in brain tissue sections of transgenic mice (APP/PS1) was evaluated in vitro with autoradiography (1). Similar to the findings obtained from staining in human AD brain tissue sections, [^125^I]71 showed specific binding with Aβ plaques (refer to the Human Studies section). No data were reported for [^125^I]70.

Cui at al. also evaluated the in vitro binding of [^125^I]71 to Aβ plaques in human AD brain tissue sections with autoradiography (1). [^125^I]71 exhibited intensive labeling of the plaques, showing strong signal in the cortex region and low background level in the white matter in the AD brain sections. The hot spots of radioactivity were consistent with the results of immunohistochemical staining in the same sections using the Aβ antibody BC05. No data were reported for [^125^I]70.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

Biodistribution studies were performed in normal mice with [^125^I]70 and [^125^I]71 (n = 4 mice/time point for each agent) (1). Both [^125^I]70 and [^125^I]71 exhibited good penetration of the BBB with excellent initial uptake in the brain (4.56% and 4.68% injected dose per gram tissue (ID/g) at 2 min, respectively), showing improved initial uptake than the previously reported radiofluorinated curcumin (0.52% ID/g at 2 min) (7). The radioactivity was then washed out rapidly (0.54% and 0.71% ID/g at 60 min for [^125^I]70 and [^125^I]71, respectively). The brain_2min_/brain_60min_ ratios were 8.44 and 6.59 for [^125^I]70 and [^125^I]71, respectively.

The thyroid uptake values for [^125^I]70 and [^125^I]71 reached 14.14% and 23.96% ID/g at 1 h, respectively, suggesting deiodination of the two agents in vivo. The two agents were cleared predominantly via the hepatobiliary system (24.17% and 23.88% ID/g in the liver at 30 min for [^125^I]70 and [^125^I]71, respectively), and the clearance was fast (25.97%–23.62% ID/g in the intestine at 60 min for [^125^I]70 and [^125^I]71, respectively). A moderate uptake of [^125^I]70 and [^125^I]71 was also observed in the kidneys (16.31% and 15.54% ID/g at 30 min, respectively), indicating that they were also excreted via the renal system.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Cui M., et al. (2011). Synthesis and structure-affinity relationships of novel dibenzylideneacetone derivatives as probes for beta-amyloid plaques. J Med Chem.
2 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
3 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
4 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
5 Frautschy S.A., et al. (2001). Phenolic anti-inflammatory antioxidant reversal of Abeta-induced cognitive deficits and neuropathology. Neurobiol Aging.
6 Lim G.P., et al. (2001). The curry spice curcumin reduces oxidative damage and amyloid pathology in an Alzheimer transgenic mouse. J Neurosci.
7 Ryu E.K., et al. (2006). Curcumin and dehydrozingerone derivatives: synthesis, radiolabeling, and evaluation for beta-amyloid plaque imaging. J Med Chem.
8 Newberg A.B., et al. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.